# (+)-(2S,3S)-3-(2-[^11^C]Methoxybenzylamino)-2-phenylpiperidine

Chemical name: | (+)-(2S,3S)-3-(2-[^11^C]Methoxybenzylamino)-2-phenylpiperidine
Abbreviated name: | [^11^C]CP-99,994
Synonym:
Agent Category: | Compound
Target: | Neurokinin 1 (NK_1_) receptor (substance P or SP receptor)
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CP-99994)]

(+)-(2S,3S)-3-(2-[^11^C}Methoxybenzylamino)-2-phenylpiperidine ([^11^C]CP-99,994) is a radioligand developed for positron emission tomography (PET) imaging of neurokinin 1 (NK_1_) receptors [substance P (SP) receptors) in the central nervous system (CNS) (1)

Tachykinins are peptides comprising 10−12 amino acids that share a common carboxy-terminal sequence “Phe-X-Gly-Leu-Met-amide” where “X” may vary but is always a hydrophobic residue that is either an aromatic or a β-branched aliphatic (2-4). This peptide family consists of SP, neurokinin A (NK_A_), and neurokinin B (NK_B_). The tachykinin peptides mediate their effects by specific G protein−coupled receptors. These receptors are divided into three subtypes: NK_1_ (formerly the SP receptor), NK_2_ (formerly the substance K/substance E receptor/NK-A receptor), and NK_3_ (formerly the NK-B receptor) receptors. The effects of SP are mediated primarily via the NK_1_ receptor subtypes. There is evidence that SP behaves like a neurotransmitter involved in regulation of emotional and behavioral responses to a range of noxious and stressful stimuli (5). SP may also play a role in neurogenic inflammation, vasomotor control, and many gastrointestinal functions. Studies in the brain have shown that SP is found in the neocortex, limbic areas, habenula, periaqueductal gray matter, midbrain nuclei, and is especially enriched in the basal ganglia. There is little SP in the cerebellum. The distribution of the NK_1_ receptors in the brain generally corresponds to that of SP.

SP-NK_1_ receptor pathways are found in both the CNS and the peripheral nervous system. The CNS pathways have been implicated in the pathophysiology of pain, nausea/emesis, and depression disorders (6). PET and single-photon emission computed tomography of radioligands that target NK_1_ receptors can visualize and allow the study of the CNS NK_1_ receptors in normal and pathologic states. These studies can identify the degree of receptor occupancy in patients with depression and the change in response to therapy (6).

Snider et al. (7) developed CP-96,345, a potent nonpeptide antagonist of the NK_1_ receptor, and showed that ^3^H-labeled CP-96,345 distributed in a similar CNS pattern similar to ^3^H-labeled SP in guinea pigs. Desai et al. (8) proposed that the position of the inner phenyl ring of the benzhydryl group relative to the C-3 benzylamino group in CP-96,345 was important for activity. On the basis of this observation, they synthesized CP-99,994, a similar nonpeptide compound with better CNS penetration. Livni et al. (1) first described the CP-99,994 radiolabeled with ^11^C as a potential PET imaging agent and evaluated its in vivo biodistribution in hamsters.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CP-99994%20AND%20synthesis)]

Desai et al. (8) reported the synthesis of CP-99,994. The enantiospecific synthesis of CP-99,994 started with the N-protection of (−)-(4R)-4-phenyl-2-azetidinone. The resulting compound was reacted with 1-bromo-3-chloropropane in a highly stereoselective alkylation to produce a β-lactam product. This was followed by simultaneous removal of the N-protection group and the hydrolysis of the β-lactam to produce an aminomethyl ester compound. Cyclization of this compound was carried out in the presence of sodium iodide and sodium bicarbonate at 100ºC for 15 min. The stereospecific conversion of the carbomethoxy group in this compound to an amino group was conducted in a four-step sequence to yield an intermediate product. Reductive amination of this intermediate product with o-methoxybenzaldehyde followed by cleavage of the Cbz group yielded CP-99,994 in the form of (+)−(2S,3S) dihydrochloric salt.

Livni et al. (1) used the CP-99,994 dihydrochloric salt to prepare the precursor for radiosynthesis of [^11^C]CP-99,994. Briefly, the hydrochloric salt was combined with concentrated hydrochloric acid, 10% palladium, methanol, and ethanol in a pressure bottle and shaken under hydrogen overnight. The resulting product was mixed and stirred in acetic acid, sodium triacetoxyborohydride and o-salicylaldehyde at room temperature for 16 h to produce (2S, 3S)-3-(2-hydroxybenzylamino)-2-phenylpiperidine. This compound was reacted with triethylamine and di-tert-butyldicarbonate in tetrahydrofuran at room temperature for 15 h to yield the precursor, (−)-(2S,3S)-1-tert-butyloxycarbonyl-3-(2-hydroxybenzylamino)-2-phenylpiperidine. In the radiosynthesis, this precursor was dissolved in dimethyl sulfoxide and then reacted with ^11^C-labeled methyl iodide in potassium hydroxide. The reaction mixture was heated at 85ºC for 8 min. After methylation of the precursor, deprotection was performed by addition of 1 N hydrochloric acid and heating at 110ºC for 2.5 min. The final product was purified by high-performance liquid chromatography. Radiochemical yield was 10% at the end of synthesis (EOS), and chemical and radiochemical purities were >95%. Specific activity at EOS was 34.7 ± 16.2 GBq/μmol (937 ± 439 mCi/μmol; n = 10), and the synthesis time was 40 min from the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CP-99994%20AND%20in%20vitro)]

Desai et al. (8) determined the in vitro binding affinity of CP-99,994 for the human NK_1_ receptor in human IM-9 cells by using [^125^I]-BH-SP, an SP antagonist. The inhibition constant (K_i_) of CP-99,994 was 0.17 ± 0.04 nM. In comparison, the K_i_ of CP-96,3435 was 0.66 ± 0.26 nM. McLean et al. (9) reported that CP-99,994 exhibited affinity that was >10,000-fold more selective for the NK_1_ receptors relative to the NK_2_ and NK_3_ receptors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CP99994%20AND%20rodentia)]

Livni et al. (1) studied the biodistribution of [^11^C]CP-99,994 in Syrian hamsters. Each animal received a dose of 370 kBq (10 μCi) by i.v. administration. There were significant levels of accumulation in most organs. The highest concentrations were found in the lung and the gastrointestinal tract. The distribution pattern was consistent with the known distribution pattern of NK_1_ receptors in these tissues. The cerebral concentration was 1.35 ± 0.16% ID/g (percentage of injected dose per gram) at 30 min after injection (n = 5−6). In comparison, the cerebral concentration of CP-96,345 was ≈0.04% ID/g.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CP-99994%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CP99994%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CP99994%20AND%20human)]

No publication is currently available.

## References

1 Livni E., Babich J.W., Desai M.C., Godek D.M., Wilkinson R.A., Rubin R.H., Fischman A.J. (1995). Synthesis of a 11C-labeled NK1 receptor ligand for PET studies. Nucl Med Biol.
2 Hietala J., Nyman M.J., Eskola O., Laakso A., Gronroos T., Oikonen V., Bergman J., Haaparanta M., Forsback S., Marjamaki P., Lehikoinen P., Goldberg M., Burns D., Hamill T., Eng W.S., Coimbra A., Hargreaves R., Solin O. (2005). Visualization and quantification of neurokinin-1 (NK1) receptors in the human brain. Mol Imaging Biol.
3 Severini C., Improta G., Falconieri-Erspamer G., Salvadori S., Erspamer V. (2002). The tachykinin peptide family. Pharmacol Rev.
4 Datar P., Srivastava S., Coutinho E., Govil G. (2004). Substance P: structure, function, and therapeutics. Curr Top Med Chem.
5 Mantyh P.W. (2002). Neurobiology of substance P and the NK1 receptor. J Clin Psychiatry.
6 Hargreaves R. (2002). Imaging substance P receptors (NK1) in the living human brain using positron emission tomography. J Clin Psychiatry.
7 Snider R.M., Constantine J.W., Lowe J.A., Longo K.P., Lebel W.S., Woody H.A., Drozda S.E., Desai M.C., Vinick F.J., Spencer R.W., Hess H.-J. (1991). A potent nonpeptide antagonist of the substance P (NK1) receptor. Science.
8 Desai M.C., Lefkowitz S.L., Thadeio P.F., Longo K.P., Snider R.M. (1992). Discovery of a potent substance P antagonist: recognition of the key molecular determinant. J Med Chem.
9 McLean S., Ganong A., Seymour P.A., Snider R.M., Desai M.C., Rosen T., Bryce D.K., Longo K.P., Reynolds L.S., Robinson G., Schmidt A.W., Siok C., Heym J. (1993). Pharmacology of CP-99,994; a nonpeptide antagonist of the tachykinin neurokinin-1 receptor. J Pharmacol Exp Ther.